# Poly(N,N-dimethylacrylamide)-coated maghemite nanoparticles for labeling and tracking mesenchymal stem cells

Chemical name: | Poly(N,N-dimethylacrylamide)-coated maghemite nanoparticles for labeling and tracking mesenchymal stem cells
Abbreviated name: | PDMAAm-coated γ-Fe_2_O_3_-labeled MSCs
Synonym: | PDMAAm-coated maghemite
Agent Category: | Cells
Target: | Others (cell imaging)
Target Category: | Non-targeted
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=mesenchymal+stem+cells+and+cell+tracking+and+imaging)]

Personalized diagnosis and treatment with allogenic or autologous cells are becoming a reality in the field of medicine (1, 2). Cytotoxic or engineered T-cells (http://clinicaltrials.gov/ct2/results?term=cytotoxic+T+cells) are under clinical trial for the treatment of hematopoietic or other malignant diseases (3). Contrast agent–tagged macrophages (http://clinicaltrials.gov/ct2/results?term=macrophage+and+imaging) are used as cellular probes to image the early inflammatory processes in macrophage-rich conditions such as inflammation, atherosclerosis, and acute cardiac graft rejection (4). The roles of stem cells (http://clinicaltrials.gov/ct2/results?term=stem+cell) are under intensive investigation in therapeutic and regenerative medicine, such as regenerating cardiomyocytes, neurons, bone, and cartilage (1). Genetically modified cells (http://clinicaltrials.gov/ct2/results?term=genetic+disorders+and+cells) are used to treat genetic disorders (5). With promising results from these studies, a critical issue is how to monitor the temporal and spatial migration and the homing of these cells, as well as the engraftment efficiency and functional capability of the transplanted cells in vivo (6, 7). Histopathological techniques have only been used to obtain information on the fate of implanted cells at the time of animal euthanization or via biopsy or surgery. To track the real-time changes of cell location, viability, and functional status, cell imaging techniques have been introduced during the last few years. Cells of interest are labeled with reporter genes, fluorescent dyes, or other contrast agents that transform the tagged cells into cellular probes or imaging agents (2, 6, 7).

The ability to monitor superparamagnetic iron oxide particles (SPIO) with magnetic resonance imaging (MRI) has been utilized in animal models as well as in a few clinical settings to investigate the fate of labeled cells (6-10). The advantages of using MRI for cell tracking include high spatial resolution with high anatomic background contrast, the lack of exposure to ionizing radiation, and the ability to follow the cells for months. In addition, cell labeling with SPIO nanoparticles is generally nontoxic and does not affect the cell proliferation and differentiation capacity, although a few studies have reported that the stem cells labeled with SPIO lose part of their differentiation capacity in a SPIO concentration–dependent manner. An important limitation of MRI is the fact that MRI signals cannot indicate whether cells are dead or alive. It is also unknown whether the MRI signal comes from targeted or labeled cells or from macrophages. Basically, SPIO particles are used to label the target cells by systemic application or by injection into the tissue area of interest to monitor target cell migration after phagocytosis. SPIO are more frequently used to label the cells in vitro by incorporating into the cells directly. Furthermore, SPIO are usually encapsulated by organic polymers to increase their stability and biocompatibility and allow the chemical modification of their surfaces. The fact is that the uptake of different particles varies largely between different cell types (6, 7).

Mesenchymal stem cells (MSCs) represent a heterogeneous subset of pluripotent stromal cells that can be isolated from different adult tissues including adipose tissue, liver, muscle, amniotic fluid, placenta, umbilical cord blood, and dental pulp, although the bone marrow remains the principal source for most preclinical and clinical studies (1, 11, 12). Although MSCs account for only 0.001–0.01% of the total nucleated cells within isolated bone marrow aspirates, they can easily be isolated and expanded in vitro through as many as 40 population doublings after 8–10 weeks of culture (1, 13). These cells exhibit the potential to differentiate into cells of diverse lineages such as adipocytes, chondrocytes, osteocytes, myoblasts, cardiomyocytes, neurons, and astrocytes. In addition, MSCs possess remarkable immunosuppressive properties and have been shown to be effective against tumor cell growth (14, 15). Babic et al. developed poly(N,N-dimethylacrylamide)-coated maghemite (PDMAAm-coated γ-Fe_2_O_3_) nanoparticles for labeling and MRI tracking of MSCs (16). Maghemite (γ-Fe_2_O_3_) nanoparticles are one of the most commonly used ferric oxide particles because of their simple synthesis and chemical stability. Because iron participates in human metabolism, ferric oxide particles are usually well tolerated by living organisms. The PDMAAm coating provides desired functional groups on the particle surface and increases the stability of the nanoparticles. PDMAAm-coated γ-Fe_2_O_3_ nanoparticles provide higher T_2_ relaxivity and better resolution than uncoated nanoprticles and Endorem. Endorem (http://www.mr-tip.com/serv1.php?type=db1&dbs=Endorem) is a commercially available MRI contrast agent that is based on dextran-coated SPIO nanoparticles (a brand name for ferumoxide).

### Relevant Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=cell+tracking+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Mesenchymal stem cells under clinical trails (http://clinicaltrials.gov/ct2/results?term=mesenchymal+stem+cells)
- SPIO and cell imaging under clinical trails (http://clinicaltrials.gov/ct2/results?term=SPIO+and+cell+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=maghemite+and+mesenchymal+stem+cells+and+poly(N,N-dimethylacrylamide))]

Babic et al. described the synthesis procedure of PDMAAm-coated maghemite nanoparticles and cell labeling in detail (16). In general, the nanoparticles were prepared in a two-step procedure. Colloidal Fe(OH)_3_ was first precipitated from FeCl_3_·6H_2_O added to less than an equimolar amount of ammonia, followed by the addition of FeCl_2_·4H_2_O (molar ratio, Fe(III)/Fe(II) = 2). The mixture was then poured into an excess of ammonia to form a magnetite (Fe_3_O_4_) coagulate. The pure magnetite was sonicated with sodium citrate solution and oxidized with sodium hypochlorite to become maghemite (Fe_2_O_3_). PDMAAm coating was achieved with a radical polymerization solution of N,N-dimethylacrylamide (DMAAm) in the presence of maghemite nanoparticles. 4,4'-Azobis(4-cyanovaleric acid) (ACVA) was preferred over 2,2'-azobisisobutyronitrile (AIBN) as an initiator for coating because of its much higher solubility in an aqueous monomer solution than that of AIBN, and because of its carboxyl group’s ability to interact with iron oxide.

The investigators then characterized the coated nanoparticles with different techniques (16). Transmission electron microscopy (TEM) showed agglomerated maghemite particles in a dry state with an iron core diameter of 6.3 nm and a polydispersity index of 1.33. The coating process did not change the shape or size of the particles. X-ray diffraction measurements demonstrated the typical spinel structure of γ-Fe_2_O_3_. The molecular weight of PDMAAm prepared in the presence of maghemite was 717.9 kDa, lower than that of PDMAAm prepared in the absence of maghemite (965.2 kDa). This can be attributed to the growing polymer chains probably terminating on the nanoparticle surface. At γ-Fe_2_O_3_/DMAAm ratios of 0.5/0.375 (w/w) and lower, free PDMAAm was present in the mixture after polymerization. The colloidal stability decreased with increasing γ-Fe_2_O_3_/DMAAm ratios. The spectrum of the nanoparticles differed from that of the pure PDMAAm, indicating that the PDMAAm shell effectively formed on the surface of the iron oxide particles. Use of ACVA as the initiator produced a very stable colloid with particles typically in the hydrodynamic size range of 50−170 nm per dynamic light scattering. While TEM provides the number-average particle size, dynamic light scattering gives the z-average, which is sensitive to large-size particles. The particles were very stable in water due to the PDMAAm coating, in that there was no increase in the hydrodynamic size and the polydispersity was consistently low over several months. The uncoated nanoparticles were unstable, showing increased hydrodynamic diameter and polydispersity over time because of aggregation. For the reaction parameters, the more DMAAm in the polymerization feed, the more PDMAAm was bound to the particles. At high ACVA amounts, the stability of the colloidal system was lost, showing aggregated particles. Both the hydrodynamic particle size and the percentage of bound PDMAAm increased with increasing amounts of the initiator up to 15 mg ACVA. Particle aggregation occurred with amounts of 1.5 g or more DMAAm in the feed, probably because of the undesirable physical cross-linking of PDMAAm chains and the increased viscosity of the reaction mixture. At a constant amount of the initiator in the feed, the percentage of PDMAAm that bound to the particles did not change with increasing amounts of DMAAm. In the case of constant particle size, the amount of bound PDMAAm decreased with increasing amounts of γ-Fe_2_O_3_ in the feed.

To investigate the effect of the PDMAAm coating on the internalization of the maghemite nanoparticles by target cells, human bone marrow MSCs (hMSCs) and rat bone marrow MSCs (rMSCs) were incubated with PDMAAm-coated nanoparticles, Endorem, or uncoated maghemite nanoparticles. hMSCs were obtained from the bone marrow of healthy donors, and rMSCs were obtained from the tibia and femur of 4-week-old Wistar rats. The same iron concentration (15 µg Fe_2_O_3_/ml in medium) of all particles was used, and incubation was carried out for 72 h. rMSCs showed considerably higher uptake of the PDMAAm-coated maghemite nanoparticles (percentage of labeled cells, 59%) than Endorem (39%). A higher uptake of PDMAAm-coated nanoparticles was observed in hMSCs (82%), whereas Endorem uptake was 68%. More cells were intensely stained with PDMAAm-coated nanoparticles than with Endorem or uncoated maghemite. The labeling efficiency was stable and was not dependent on the number of cell passages (16).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=maghemite+and+mesenchymal+stem+cells+and+poly(N,N-dimethylacrylamide))]

Babic et al. first evaluated the acute toxicity of PDMAAm-coated maghemite nanoparticles after incubation of the rMSCs and hMSCs with the nanoparticles for 72 h at a concentration of 15 µg γ-Fe_2_O_3_/ml (16). The cell viability of both rat and human labeled MSCs did not markedly decrease compared with that of unlabeled MSCs (control). When the MSCs were labeled with Endorem, cell viability decreased by 32% and by 15% with uncoated maghemite nanoparticles. The TEM images showed that cells internalized the PDMAAm-coated nanoparticles in large numbers and accumulated them in endosomes. Organelles and cell structures were not affected. MSCs labeled with Endorem showed a heterogeneous distribution of the nanoparticles. Some of the cells contained numerous endosomes filled with nanoparticles; others contained only a few or none. The majority of the cells labeled with uncoated maghemite underwent programmed cell death, probably by autophagia.

Babic et al. then analyzed the relaxometry after dispersing the labeled cells in gelatin at concentrations of 50, 100, 200, 400, and 800 cells/µl, separately (16). Relaxation rates r_1_ and r_2_ were related to the number of cells/µl. PDMAAm-coated maghemite-labeled hMSCs provided significantly higher r_1_ and r_2_ rates than Endorem- and uncoated maghemite–labeled cells. Large differences were observed for the relaxation rates between PDMAAm-labeled human and rat cells, with r_2_ nearly 10 times higher for human cells. PDMAAm-coated maghemite-labeled rat cells provided higher relaxation rates than Endorem-labeled cells; however, they were quite comparable to uncoated maghemite–labeled cells. These results indicated that human cells preferred PDMAAm-coated nanoparticles to both Endorem and uncoated ones, whereas in the case of rat cells, uncoated iron particles were internalized at slightly higher rates than PDMAAm-coated ones. Similarly, the T_2_- and T_2_*-weighted MRI of gelatin showed that cells labeled with PDMAAm-coated maghemite nanoparticles had higher negative contrast enhancement than cells labeled with Endorem or unlabeled cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=maghemite+and+mesenchymal+stem+cells+and+poly(N,N-dimethylacrylamide))]

In vivo MRI was performed on a 4.7-T imager after implantation of PDMAAm-coated maghemite-labeled cells and Endorem-labeled cells (5,000 cells suspended in 5 µl phosphate-buffered saline) into the left and right rat brain hemispheres, respectively (n = 5 rats). Unlabeled cells were injected as a control. Only cells labeled with PDMAAm-coated maghemite nanoparticles were detected (16).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Mathiasen A.B., Haack-Sorensen M., Kastrup J. (2009). Mesenchymal stromal cells for cardiovascular repair: current status and future challenges. Future Cardiol.
2 Arbab A.S., Janic B., Haller J., Pawelczyk E., Liu W., Frank J.A. (2009). In Vivo Cellular Imaging for Translational Medical Research. Curr Med Imaging Rev.
3 Cesco-Gaspere M., Morris E., Stauss H.J. (2009). Immunomodulation in the treatment of haematological malignancies. Clin Exp Med.
4 Eisenblatter M., Ehrchen J., Varga G., Sunderkotter C., Heindel W., Roth J., Bremer C., Wall A. (2009). In vivo optical imaging of cellular inflammatory response in granuloma formation using fluorescence-labeled macrophages. J Nucl Med.
5 Bachoud-Levi A.C. (2009). Neural grafts in Huntington's disease: viability after 10 years. Lancet Neurol.
6 Himmelreich U., Dresselaers T. (2009). Cell labeling and tracking for experimental models using magnetic resonance imaging. Methods.
7 Hoehn M., Wiedermann D., Justicia C., Ramos-Cabrer P., Kruttwig K., Farr T., Himmelreich U. (2007). Cell tracking using magnetic resonance imaging. J Physiol.
8 Park, K.S., J. Tae, B. Choi, Y.S. Kim, C. Moon, S.H. Kim, H.S. Lee, J. Kim, J.S. Kim, J. Park, J.H. Lee, J.E. Lee, J.W. Joh, and S. Kim, Characterization, in vitro cytotoxicity assessment, and in vivo visualization of multimodal, RITC-labeled, silica-coated magnetic nanoparticles for labeling human cord blood-derived mesenchymal stem cells. Nanomedicine, 2010
9 Wang H.H., Wang Y.X., Leung K.C., Au D.W., Xuan S., Chak C.P., Lee S.K., Sheng H., Zhang G., Qin L., Griffith J.F., Ahuja A.T. (2009). Durable mesenchymal stem cell labelling by using polyhedral superparamagnetic iron oxide nanoparticles. Chemistry.
10 Yoon T.J., Kim J.S., Kim B.G., Yu K.N., Cho M.H., Lee J.K. (2005). Multifunctional nanoparticles possessing a "magnetic motor effect" for drug or gene delivery. Angew Chem Int Ed Engl.
11 Ehrchen J., Helming L., Varga G., Pasche B., Loser K., Gunzer M., Sunderkotter C., Sorg C., Roth J., Lengeling A. (2007). Vitamin D receptor signaling contributes to susceptibility to infection with Leishmania major. FASEB J.
12 Sadan O., Melamed E., Offen D. (2009). Bone-marrow-derived mesenchymal stem cell therapy for neurodegenerative diseases. Expert Opin Biol Ther.
13 Huang D.M., Hsiao J.K., Chen Y.C., Chien L.Y., Yao M., Chen Y.K., Ko B.S., Hsu S.C., Tai L.A., Cheng H.Y., Wang S.W., Yang C.S. (2009). The promotion of human mesenchymal stem cell proliferation by superparamagnetic iron oxide nanoparticles. Biomaterials.
14 Loebinger M.R., Kyrtatos P.G., Turmaine M., Price A.N., Pankhurst Q., Lythgoe M.F., Janes S.M. (2009). Magnetic resonance imaging of mesenchymal stem cells homing to pulmonary metastases using biocompatible magnetic nanoparticles. Cancer Res.
15 Kuhn N.Z., Tuan R.S. (2010). Regulation of stemness and stem cell niche of mesenchymal stem cells: implications in tumorigenesis and metastasis. J Cell Physiol.
16 Babic M., Horak D., Jendelova P., Glogarova K., Herynek V., Trchova M., Likavanova K., Lesny P., Pollert E., Hajek M., Sykova E. (2009). Poly(N,N-dimethylacrylamide)-coated maghemite nanoparticles for stem cell labeling. Bioconjug Chem.